# Quantum dot 800-conjugated anti-Tn IgM 2154F12A4 murine monoclonal antibody

Chemical name: | Quantum dot 800-conjugated anti-Tn IgM 2154F12A4 murine monoclonal antibody
Abbreviated name: | Qdot 800-anti-Tn 2154F12A4 mAb
Synonym:
Agent Category: | Antibody
Target: | Tumor-associated carbohydrate Tn antigen
Target Category: | Antigen
Method of detection: | Near-infrared fluorescence optical imaging
Source of signal / contrast: | Quantum dot 800
Activation: | No
Studies: | - In vitro; - Rodents | No structure available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Tn%20antigen%20and%20antibody%20)]

The Tn-antigen is a tumor-associated carbohydrate epitope (N-acetyl-galactosamine (GalNAc)-O-Ser/Thr (GalNAca-O-Ser/Thr)) (1-3). The anti-Tn 2154F12A4 murine monoclonal antibody (mAb) and its quantum dot (Qdot) 800 conjugate (Qdot 800-anti-Tn 2154F12A4 mAb) were developed by Danussi et al. for in vivo imaging and immunotherapy of Tn-expressing tumors (4).

Qdots are nanometer-sized crystals (typically 2–10 nm in diameter) (5-7). In contrast to organic fluorophores, Qdots have a continuous absorption spectrum for wavelengths shorter than the wavelengths of fluorescence emission. The emission spectra are quite narrow and symmetric. Many different colors can be excited with one wavelength of excitation, and the colors can be spectrally well resolved. Qdots exhibit good quantum yields (40–90%) and high extinction coefficients, and they are 20 times as bright as and 100 times as stable against photobleaching as conventional fluorophores. Qdots can be coated with hydrophilic materials and functionalized with antibodies, peptides, nucleic acids, and various compounds. Because of these unique photophysical properties, Qdots have been intensively investigated as biosensors and labels in biological imaging (5-7). However, most Qdots are toxic (8). The most widely used and studied Qdots consist of a core of cadmium selenide or telluride because their quantum confinement regions span the entire optical spectrum. Cadmium ions are able to bind to thiol groups on critical molecules in the mitochondria to cause significant cell death. Qdots may also damage DNA and disrupt normal cell activity from factors such as the surface coatings themselves (8).

Altered glycosylation on the cell surface is a hallmark of malignant transformation and tumor progression. Incomplete synthesis of the carbohydrate chains and precursor accumulation result in loss of the normal carbohydrate antigens and high expression of the tumor-associated carbohydrate antigens (9-11). Lewis Y, TF, Globo H, GM2, polysialic acid, sialyl Lewis A, Tn, and sialyl Tn are some of the antigens investigated intensively as diagnostic markers or as vaccine antigens (10-13). The Tn antigen was first reported as a tumor-associated antigen nearly 40 years ago (14). It is composed of a single GalNAc glycan residue attached via an α-linkage to either the serine (Ser) or the threonine (Thr) of a polypeptide chain (11, 13). In normal tissues, the Tn antigen is generally masked by covalently bound terminal carbohydrate moieties, but in tumors it is unmasked because of defective O-glycosylation. Accordingly, the Tn antigen is rarely expressed in normal tissues, but it is widely expressed in human carcinomas or hematological cancers. It has been reported that the Tn antigen is expressed in 70–90% of breast, colon, lung, bladder, cervical, ovarian, stomach, and prostate tumors (1, 3, 9). The expression levels of the Tn antigen are closely associated with tumor aggressiveness and poor survival of patients (10, 12). In addition, the Tn antigen is recognized by the human immune system as a novel epitope, provoking immune responses in patients. There is a strong correlation among the expression of the Tn antigen, the development of the spontaneous antibodies against Tn, and the prognosis of patients with carcinomas. Clinical trials (http://clinicaltrials.gov/ct2/results?term=Tn+and+vaccine) are under way to deliberately provoke or enhance human immune responses by injecting patients with synthetic peptide antigens bearing Tn structure (3, 10, 15-17).

The Tn antigen has attracted significant interest as a target for tumor diagnosis and immunotherapy. A number of anti-Tn IgG and IgM antibodies have been generated and investigated for their imaging feasibilities and anti-tumor activities (2, 18-25). The results are generally inconsistent. There are still some issues to be resolved, such as immunogenicity, reduced effectiveness in vivo, and cross-reactivity against type-A blood antigen. Danussi et al. developed an anti-Tn IgM mAb and further tested its imaging feasibility and antitumor activity (4).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Tn%20antigen%20and%20antibody%20and%20imaging)]

The anti-Tn 2154F12A4 IgM mAb was synthesized by Danussi et al. on the basis of the strategy of Tn-antigen clusterization with different polymeric scaffolds and stepwise selection of the most reactive antibody-producing clones (4). The synthesis could be generally divided into synthesis of the Tn antigen (glycoamino acid GalNAc-α-O-Ser), immunization of the mice, and selection of effective clones. Briefly, 2-azido-2-deoxy-1,3,4,6-tetra-O-acetyl galactose was selectively deacetylated at the anomeric position with hydrazine hydrate, which was further converted into trichloroacetimidate (CCl_3_CN/CH_2_Cl_2_). The activated sugar was then conjugated to N-benzyloxycarbonyl-L-serine benzylester, giving rise to the anomeric mixture after removal of the protecting groups. The global yield of the Tn antigen (glycoaminoacid) mixture was 20%, and the α-form of the Tn antigen accounted for 65% of the mixture, which was purified with high-performance liquid chromatography. For immunizing mice, the glycoaminoacid was conjugated with cationic bovine serum albumin (cBSA); and for titrating serum and selecting anti-Tn clones, the glycoaminoacid was labeled with biotinylated alginate. To produce the specific antibody, three series of immunization were performed on BALB/c mice (n = 2 in each series) with intraperitoneal injection of the Tn-cBSA conjugates once a week for 3 weeks, followed by boosts with three daily additional intravenous injections of the antigen after 1 month. To obtain effective mAb-producing clones, the animals were euthanized after immunization, and the spleen cells were fused with mouse myeloma NS1 cells. The hybrid cells were cultured in glucose-modified Dulbecco’s medium, and clones were selected with hypoxanthine aminopterin thymidine medium. The antibodies produced from the clone 2154F12A4 showed the highest and most efficient binding for Tn antigen as described below. The detailed procedure for the conjugation of 2154F12A4 mAb to Qdot 800 was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Tn%20antigen%20and%20antibody%20and%20imaging)]

The binding specificity of the 2154F12A4 mAb for Tn antigen was analyzed with immobilized antigen enzyme-linked immunosorbent assay, immunofluorescent staining of the MCF7 human breast cancer cells, and solid-phase preclearing test (4). Their results showed that the 2154F12A4 mAb selectively and efficiently recognized the Tn antigen immobilized as well as on the MCF7 cell surface. Preincubation of the mAb with purified Tn antigen abolished the binding of the mAb with MCF7 cells in a manner dependent on the Tn antigen dose (P < 0.001).

Danussi et al. further investigated whether the 2154F12A4 mAb affected the adhesion of MCF7 cells to lymphatic endothelial cells (4). The fluorescently labeled MCF7 cells (vital fluorochrome calcein acetoxymethyl ester) were pretreated with the 2154F12A4 mAb or with the isotype control IgM antibody for 20 min before the cells were seeded into the human microvascular endothelial cells–lung lymphatic (HMVEC-LLy)-coated plates. Treatment of the cells with the 2154F12A4 mAb significantly inhibited the breast cancer cell adhesion on the HMVEC-LLy cells up to 30% (P = 0.002), indicating that the Tn antigen is implicated in the molecular mechanism of lymphatic metastasis of tumors.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Tn%20antigen%20and%20antibody%20and%20imaging)]

Optical imaging with the Qdot 800-anti-Tn 2154F12A4 mAb (50 µg, administered via the tail vein) was performed on mice bearing subcutaneous MCF7 tumor xenografts. Whole-animal imaging showed that the Qdot 800-anti-Tn 2154F12A4 mAb accumulated in and strongly stained the flank tumor mass as well as the homolateral inguinal lymph nodes at 72 h after injection. Consistent with the in vivo imaging results, the ex vivo imaging also showed a higher level of fluorescence signal in the homolateral than in the heterolateral inguinal and axillary lymph nodes, suggesting the presence of the MCF7 metastatic cells in the draining lymph nodes. Immunohistochemistry with an anti-pan cytokeratin antibody, a specific marker of epithelial as well as of carcinoma cells, confirmed the presence of the tumor cells in the homolateral lymph nodes. The fluorescent signal from the lung, liver, kidneys, and spleen were all negligible. The detailed biodistribution data of the Qdot 800-anti-Tn 2154F12A4 mAb were not reported.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Springer G.F. (1997). Immunoreactive T and Tn epitopes in cancer diagnosis, prognosis, and immunotherapy. J Mol Med.
2 Ando H., Matsushita T., Wakitani M., Sato T., Kodama-Nishida S., Shibata K., Shitara K., Ohta S. (2008). Mouse-human chimeric anti-Tn IgG1 induced anti-tumor activity against Jurkat cells in vitro and in vivo. Biol Pharm Bull.
3 Li Q., Anver M.R., Butcher D.O., Gildersleeve J.C. (2009). Resolving conflicting data on expression of the Tn antigen and implications for clinical trials with cancer vaccines. Mol Cancer Ther.
4 Danussi C., Coslovi A., Campa C., Mucignat M.T., Spessotto P., Uggeri F., Paoletti S., Colombatti A. (2009). A newly generated functional antibody identifies Tn antigen as a novel determinant in the cancer cell-lymphatic endothelium interaction. Glycobiology.
5 Walling M.A., Novak J.A., Shepard J.R. (2009). Quantum dots for live cell and in vivo imaging. Int J Mol Sci.
6 Drbohlavova J., Adam V., Kizek R., Hubalek J. (2009). Quantum dots - characterization, preparation and usage in biological systems. Int J Mol Sci.
7 Bentolila L.A., Ebenstein Y., Weiss S. (2009). Quantum dots for in vivo small-animal imaging. J Nucl Med.
8 Rzigalinski B.A., Strobl J.S. (2009). Cadmium-containing nanoparticles: perspectives on pharmacology and toxicology of quantum dots. Toxicol Appl Pharmacol.
9 Babino A., Oppezzo P., Bianco S., Barrios E., Berois N., Navarrete H., Osinaga E. (2000). Tn antigen is a pre-cancerous biomarker in breast tissue and serum in n-nitrosomethylurea-induced rat mammary carcinogenesis. Int J Cancer.
10 Hakomori S. (2001). Tumor-associated carbohydrate antigens defining tumor malignancy: basis for development of anti-cancer vaccines. Adv Exp Med Biol.
11 Kulkarni K.A., Sinha S., Katiyar S., Surolia A., Vijayan M., Suguna K. (2005). Structural basis for the specificity of basic winged bean lectin for the Tn-antigen: a crystallographic, thermodynamic and modelling study. FEBS Lett.
12 Kurtenkov O., Klaamas K., Rittenhouse-Olson K., Vahter L., Sergejev B., Miljukhina L., Shljapnikova L. (2005). IgG immune response to tumor-associated carbohydrate antigens (TF, Tn, alphaGal) in patients with breast cancer: impact of neoadjuvant chemotherapy and relation to the survival. Exp Oncol.
13 Lescar J., Sanchez J.F., Audfray A., Coll J.L., Breton C., Mitchell E.P., Imberty A. (2007). Structural basis for recognition of breast and colon cancer epitopes Tn antigen and Forssman disaccharide by Helix pomatia lectin. Glycobiology.
14 Dausset J., Moullec J., Bernard J. (1959). Acquired hemolytic anemia with polyagglutinability of red blood cells due to a new factor present in normal human serum (Anti-Tn). Blood.
15 Springer G.F., Desai P.R., Spencer B.D., Tegtmeyer H., Carlstedt S.C., Scanlon E.F. (1995). T/Tn antigen vaccine is effective and safe in preventing recurrence of advanced breast carcinoma. Cancer Detect Prev.
16 Slovin S.F., Ragupathi G., Musselli C., Olkiewicz K., Verbel D., Kuduk S.D., Schwarz J.B., Sames D., Danishefsky S., Livingston P.O., Scher H.I. (2003). Fully synthetic carbohydrate-based vaccines in biochemically relapsed prostate cancer: clinical trial results with alpha-N-acetylgalactosamine-O-serine/threonine conjugate vaccine. J Clin Oncol.
17 Cipolla L., Rescigno M., Leone A., Peri F., La Ferla B., Nicotra F. (2002). Novel Tn antigen-containing neoglycopeptides: synthesis and evaluation as anti tumor vaccines. Bioorg Med Chem.
18 Takahashi H.K., Metoki R., Hakomori S. (1988). Immunoglobulin G3 monoclonal antibody directed to Tn antigen (tumor-associated alpha-N-acetylgalactosaminyl epitope) that does not cross-react with blood group A antigen. Cancer Res.
19 Yao Z., Sakahara H., Zhang M., Kobayashi H., Nakada H., Yamashina I., Konishi J. (1995). Radioimmunoimaging of colon cancer xenografts with anti-Tn monoclonal antibody. Nucl Med Biol.
20 Yao Z., Zhang M., Sakahara H., Saga T., Kobayashi H., Nakamoto Y., Toyama S., Konishi J. (1998). Increased streptavidin uptake in tumors pretargeted with biotinylated antibody using a conjugate of streptavidin-fab fragment. Nucl Med Biol.
21 Zhang M., Yao Z., Saga T., Sakahara H., Nakamoto Y., Sato N., Nakada H., Yamashina I., Konishi J. (1998). Improved intratumoral penetration of radiolabeled streptavidin in intraperitoneal tumors pretargeted with biotinylated antibody. J Nucl Med.
22 Zhang M., Yao Z., Sakahara H., Saga T., Nakamoto Y., Sato N., Zhao S., Nakada H., Yamashina I., Konishi J. (1998). Effect of administration route and dose of streptavidin or biotin on the tumor uptake of radioactivity in intraperitoneal tumor with multistep targeting. Nucl Med Biol.
23 Nakamoto Y., Saga T., Sakahara H., Yao Z., Zhang M., Sato N., Zhao S., Nakada H., Yamashina I., Konishi J. (1998). Three-step tumor imaging with biotinylated monoclonal antibody, streptavidin and 111In-DTPA-biotin. Nucl Med Biol.
24 Numata Y., Nakada H., Fukui S., Kitagawa H., Ozaki K., Inoue M., Kawasaki T., Funakoshi I., Yamashina I. (1990). A monoclonal antibody directed to Tn antigen. Biochem Biophys Res Commun.
25 Oppezzo P., Osinaga E., Tello D., Bay S., Cantacuzene D., Irigoin F., Ferreira A., Roseto A., Cayota A., Alzari P., Pritsch O. (2000). Production and functional characterization of two mouse/human chimeric antibodies with specificity for the tumor-associated Tn-antigen. Hybridoma.